# IRDye800-2-Deoxy-D-glucose

Chemical name: | IRDye800-2-Deoxy-D-glucose
Abbreviated name: | IRDye800-2-DG
Synonym:
Agent category: | Compound
Target: | Glucose transporters, hexokinases
Target category: | Transporter, enzyme
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | IRDye800
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IRDye800-2-DG)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive complement to radionuclide imaging in small animals.

The phosphorylation of glucose, an initial and important step in cellular metabolism, is catalyzed by hexokinases (HKs) (4). There are four HKs in mammalian tissues (HKI–HKIV). HKI, HKII, and HKIII have molecular weights of ~100,000 each; HKI is found mainly in the brain, and HKII is insulin-sensitive and is found in adipose and muscle cells. HKIV, also known as glucokinase, has a molecular weight of 50,000 and is specific to the liver and pancreas. Most brain HK is bound to mitochondria, enabling coordination between glucose consumption and oxidation. Tumor cells are known to be highly glycolytic because of increased expression of glycolytic enzymes and HK activity (5), which was detected in tumors from patients with lung, gastrointestinal, and breast cancers. The HKs, by converting glucose to glucose-6-phosphate, help maintain the downhill gradient that results in the transport of glucose into cells through the facilitative glucose transporters (GLUT1–13) (6). GLUT4 and HKII are the major transporters and HK isoforms in skeletal muscle, heart, and adipose tissue, wherein insulin promotes glucose utilization. HKIV is associated with GLUT2 in liver and pancreatic β cells.

2-Deoxy-D-glucose (2-DG) was first developed to inhibit glucose utilization by cancer cells (7). HKs phosphorylate 2-DG to 2-DG-6-phosphate, which inhibits phosphorylation of glucose. 2-[^18^F]Fluoro-2-deoxy-D-glucose ([^18^F]FDG) was later developed for molecular imaging studies (8). FDG is moved into cells by glucose transporters and is then phosphorylated by HK to FDG-6-phosphate. FDG-6-phosphate cannot be metabolized further in the glycolytic pathway and remains in the cells. Tumor cells do not contain a sufficient amount of glucose-6-phosphatase to reverse the phosphorylation. The elevated rates of glycolysis and glucose transport in many types of tumor cells and activated cells enhance the uptake of FDG in these cells relative to other normal cells. Positron emission tomography (PET) with [^18^F]FDG has been used to assess alterations in glucose metabolism in brain, cancer, cardiovascular diseases, Alzheimer’s disease and other central nervous system disorders, and infectious, autoimmune, and inflammatory diseases (9-14). Kovar et al. (15) developed a NIR-labeled 2-DG (IRDye800-2-DG) with IRDye800 by conjugation of IRDye800 to 2-amino-2-DG. IRDye800-2-DG is being evaluated as an optical imaging agent for in vivo imaging of tumors in mice.

### Related Resource Links:

- Chapters in MICAD (Hexokinase (http://www.ncbi.nlm.nih.gov/books?term=(hexokinase%20OR%20hexokinases)%20AND%20micad%5Bbook%5D), glucose transporter (http://www.ncbi.nlm.nih.gov/books?term=glucose%20transporters%20%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Hexokinase (http://www.ncbi.nlm.nih.gov/gene?term=hexokinase%20human), Glut1 (http://www.ncbi.nlm.nih.gov/gene/6513)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (Hexokinase (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hexokinase%5BAll+Fields%5D), Glut1 (http://www.ncbi.nlm.nih.gov/omim/138140))
- Clinical trials ([^18^F]FDG (http://www.clinicaltrials.gov/ct2/results?term=FDG))
- Drug information in FDA ([^18^F]FDG (http://google2.fda.gov/search?q=%5B18F%5DFDG&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=9))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IRDye800-2-DG+synthesis)]

IRDye800CW-N-Hydroxysuccinimide ester (LI-COR, Lincoln, NE) was reacted with 2-amino-2-DG for 2 h at room temperature in 1 M potassium phosphate buffer (pH 8.5) (15). IRDye800-2-DG was purified with high-performance liquid chromatography and verified with NMR spectroscopy.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IRDye800-2-DG+in+vitro)]

In vitro uptake studies of IRDye800-2-DG were performed with A431, 3T3-L1, and 22Rv1 cells in culture showing that high, medium, and low NIR fluorescence intensity correlated with their metabolic activity, respectively (15). Monoclonal antibody against GLUT1, D-glucose, or 2-DG was able to block the uptake of IRDye800-2-DG in a dose-dependent manner. Fluorescence microscopy showed that IRDye800-2-DG accumulated in the cytoplasm of several tumor cells (M21-L melanoma and MDA-MB-231 breast carcinoma cell lines) but was not localized in the cell surface and nucleus. Excess 2-DG was able to block the NIR fluorescence signal in the cytoplasm.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IRDye800-2-DG+rodentia)]

Kovar et al. (15) performed in vivo NIR fluorescence imaging studies of IRDye800-2-DG and IRDye800 (20 nmol per mouse) in mice bearing VEGFR-2–expressing 22Rv1 xenografts. Sagittal images were obtained at 18, 24, 30, 42, and 72 h after intravenous injection. IRDye800-2-DG exhibited peak signal intensity at 18 h with a gradual washout. There was a four-fold increase in signal over IRDye800 at 24 h after injection. Ex vivo NIR fluorescence images of various organs were obtained at 24 and 36 h after injection. IRDye800-2-DG exhibited NIR intensities one to three times higher than did IRDye800 in the kidney, lung, muscle, and liver at 24 h. The brain, spleen, intestine, and heart exhibited only background signal. All organs showed minimal NIR intensities by 36 h with either IRDye800-2-DG or IRDye800 injection, whereas the tumor showed ~1-fold higher signal with IRDye800-2-DG injection compared with IRDye800 injection. Other tumor xenografts showed varied uptake dependent on cellular origin of the tumors at 24 h after injection. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IRDye800-2-DG+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IRDye800-2-DG+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IRDye800-2-DG+human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Smith T.A. (2000). Mammalian hexokinases and their abnormal expression in cancer. Br J Biomed Sci.
5 Suolinna E.M., Haaparanta M., Paul R., Harkonen P., Solin O., Sipila H. (1986). Metabolism of 2-[18F]fluoro-2-deoxyglucose in tumor-bearing rats: chromatographic and enzymatic studies. Int J Rad Appl Instrum B.
6 Avril N. (2004). GLUT1 expression in tissue and (18)F-FDG uptake. J Nucl Med.
7 Laszlo J., Humphreys S.R., Goldin A. (1960). Effects of glucose analogues (2-deoxy-D-glucose, 2-deoxy-D-galactose) on experimental tumors. J Natl Cancer Inst.
8 Fowler J.S., Ido T. (2002). Initial and subsequent approach for the synthesis of 18FDG. Semin Nucl Med.
9 Phelps M.E. (2000). PET: the merging of biology and imaging into molecular imaging. J Nucl Med.
10 Phelps M.E., Mazziotta J.C. (1985). Positron emission tomography: human brain function and biochemistry. Science.
11 Phelps M.E., Mazziotta J.C., Huang S.C. (1982). Study of cerebral function with positron computed tomography. J Cereb Blood Flow Metab.
12 Rohren E.M., Turkington T.G., Coleman R.E. (2004). Clinical applications of PET in oncology. Radiology.
13 Sokoloff L. (1985). Basic principles in imaging of regional cerebral metabolic rates. Res Publ Assoc Res Nerv Ment Dis.
14 Spence A.M., Mankoff D.A., Muzi M. (2003). Positron emission tomography imaging of brain tumors. Neuroimaging Clin N Am.
15 Kovar J.L., Volcheck W., Sevick-Muraca E., Simpson M.A., Olive D.M. (2009). Characterization and performance of a near-infrared 2-deoxyglucose optical imaging agent for mouse cancer models. Anal Biochem.